# Activatable Alexa Fluor680-conjugated panitumumab and indocyanine green-conjugated trastuzumab cocktail

Chemical name: | Activatable Alexa Fluor680-conjugated panitumumab and indocyanine green-conjugated trastuzumab cocktail
Abbreviated name: | Pan-Alexa680 and Tra-ICG cocktail
Synonym:
Agent Category: | Antibodies
Target: | Human epidermal growth factor receptor type 1 (EGFR, HER1) and type 2 (HER2)
Target Category: | Receptors
Method of detection: | Optical imaging
Source of signal / contrast: | Indocyanine green (ICG) and Alexa Fluor680
Activation: | Yes
Studies: | - In vitro; - Rodents | No structures are available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=optical%20imaging%20and%20antibody%20and%20avtivatable)]

The cocktail of activatable Alexa Fluor680 (Alexa680)-conjugated panitumumab (Pan) and indocyanine green (ICG)-conjugated trastuzumab (Tra) is a mixture of two self-quenched (SQ), activatable monoclonal antibody (mAb) probes (abbreviated as Pan-Alexa680 and Tra-ICG, respectively) that was developed by Sano et al. for multicolor optical imaging of breast cancer (1).

mAbs are widely used to develop optical imaging probes because of their high specificity and affinity to target antigens. However, use of intact mAbs as imaging probes has some disadvantages, such as slow clearance from body, which results in high background and slow penetration of solid tumors (2, 3). To overcome this issue, activatable or “smart” fluorescent probes have been engineered to be silent (fluorescence quenching) but emit signal when or after binding with antigens in the tissue of interest (4, 5).

Several photochemical mechanisms of fluorescence quenching and activation have been proposed in the literature, such as homo- (SQ) and hetero-Förster resonance energy transfer (FRET), autoquenching, dimer formation, and photon-induced electron transfer (PeT) (2, 6, 7). Self-quenching of the fluorescence occurs when two excited fluorophores of the same molecule are close enough (<10 nm) to enable them to absorb energy from each other. Hetero-FRET refers to the quenching that occurs between two fluorophores from different molecules (a fluorophore and a quencher molecule). Autoquenching has been observed for some compounds, which can spontaneously induce a quenched state when conjugated with proteins. Autoquenching appears to be induced by the interactions between fluorophores and aromatic rings of amino acids. ICG is a dye that can be fully autoquenched when it is covalently conjugated with mAbs via the side chain of lysine, even at a low conjugation ratio. Some compounds can form H- or J-homodimers at high concentrations (~mM) in aqueous solutions and quench the emission fluorescence signal. PeT is used for the fluorescence quenching that happens within a single fluorophore molecule that is engineered to contain two parts, with one part acting as the PeT donor and another part acting as the fluorophore. Electron transfer from the PeT donor to the excited fluorophore diminishes the fluorescence signal, and cleavage of the PeT donor leads to full activation of the fluorophore. In reality, some activatable probes are designed on the basis of two or more mechanisms of fluorescent quenching and activation (8).

The activatable probes published to date can be classified into two types based on the location of fluorophore activation (2). One type involves enzymatic activation of the probes through cleavage by the extracellular or cell surface enzymes. This type of probe produces fluorescent signal primarily in the extracellular space. Another type of probe, known as a target cell–specific activatable probe, is quenched until activated through the lysosomal processing within targeted cells. Therefore, this type of probe generates fluorescent signal within the target cells. Regardless of the types, an important parameter that must be optimized for many activatable probes is the number of conjugated fluorophores per single mAb molecule. The number of conjugated fluorophores not only determines whether the fluorescence is “always on” or “silent,” but it also influences the binding specificity and in vivo pharmacokinetics (1, 2).

Sano et al. labeled two different antibodies, Pan and Tra, with activatable near-infrared Alexa680 and ICG, respectively (1). Pan is a fully human IgG2 mAb against the extracellular domain of human epidermal growth factor receptor (EGFR, HER1), and Tra is a recombinant humanized mAb against the human EGFR type 2 (HER2). The two fluorescent dyes emit light at different wavelengths (650/702 nm and 780/820 nm for Alexa680 and ICG, respectively). The investigators administered the two activatable antibodies as a cocktail to mice bearing tumor xenografts and demonstrated the feasibility of multicolor target-specific fluorescence imaging with reduced background noise (1).

### Related Resource Links:

EGFR- and HER2-targeted imaging agents (http://www.ncbi.nlm.nih.gov/books/?term=EGFR+and+HER2+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=EGFR) and protein (http://www.ncbi.nlm.nih.gov/protein?term=EGFR) sequences of EGFR

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=HER2) and protein (http://www.ncbi.nlm.nih.gov/protein?term=HER2) sequences of HER2

EGFR-related clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFR) in ClinicalTrials.gov

HER2-related clinical trials (http://clinicaltrials.gov/ct2/results?term=human+epidermal+growth+factor+receptor+type+2+%28HER2%29) in ClinicalTrials.gov

Bioassays of EGFR (http://www.ncbi.nlm.nih.gov/pcassay?term=EGFR) and HER2 (http://www.ncbi.nlm.nih.gov/pcassay?term=HER2) in PubChem

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22510481)]

Pan and Tra are commercially available. Fluorescent labeling was achieved by incubating Pan and Tra with Alexa680-NHS ester and ICG, respectively (1). The concentrations of Alexa680 and ICG were calculated by measuring the absorption with a UV-Vis system to confirm the number of fluorophore molecules conjugated to each mAb molecule. The numbers of Alexa680 and ICG molecules per mAb were adjusted to ~4.0–4.5 and 0.7–1.0, respectively, for SQ, activatable Pan-Alexa680(SQ) and Tra-ICG. As a comparison, Pan conjugated with ~1 Alexa680 molecule (always-on (ON) type; Pan-Alexa680(ON)) was also synthesized.

The quenching ability of each conjugate was evaluated by denaturing them with 1% sodium dodecyl sulfate in phosphate-buffered saline (PBS) for 15 min at room temperature (1). The results showed that the quenching capacities were 50-, 5.2-, and 1.2-fold for Tra-ICG, Pan-Alexa680(SQ), and Pan-Alexa680(ON), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22510481)]

In vitro characterization of the probe fluorescence was performed with EGFR+/HER2– breast cancer cell line MDA-MB-468 and EGFR–/HER2+ cell line NIH/3T3 (3T3/HER2) after incubation of the cells with each probe (10 µg) for 1 h and 8 h (1).

Under microscopy, the fluorescent signal from both Pan-Alexa680(ON) and Pan-Alexa680(SQ) was observed on the surface of MDA-MB-468 cells at 1 h and within the cells at 8 h after incubation. The fluorescent signal was stronger for Pan-Alexa680(SQ) than for Pan-Alexa680(ON). The signal could be completely blocked by addition of excess Pan (100 µg). For Tra-ICG, the fluorescence signal was observed within the 3T3/HER2 cells. The fluorescent signal was minimal at 1 h (due to the greater quenching magnitude of Tra-ICG than Pan-Alexa680) and became stronger over time after incubation. The signal of Tra-ICG could be blocked by addition of excess Tra (100 µg).

Flow cytometry studies also showed fluorescent signal from Pan-Alexa680(ON), Pan-Alexa680(SQ), and Tra-ICG in MDA-MB-468 and 3T3/HER2 cells, respectively. Pan-Alexa680(SQ) and Tra-ICG showed progressively brighter signal over time compared with Pan-Alexa680(ON), which showed lower and constant signal.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22510481)]

In vivo two-color imaging was performed in mice bearing tumor xenografts of MDA-MB-468 and 3T3/HER2 (n = 4 mice/group per time point). A cocktail of Tra-ICG and Pan-Alexa680(SQ) or Pan-Alexa680(ON) (50 μg each) was injected via the tail vein (1). Images were obtained with a fluorescence camera with two filter sets for Alexa680 and ICG, respectively.

Images showed accumulation of Pan-Alexa680(ON) in the targeted MDA-MB-468 tumors (EGFR+), with high background and non-specific uptake in the 3T3/HER2 tumors on day 1 through day 3 after injection. On day 4, relatively selective accumulation in MDA-MB-468 tumors was obtained. In contrast, images obtained with Pan-Alexa680(SQ) clearly showed MDA-MB-468 tumors with high tumor/background ratios from day 2, although weak signal was detected in the 3T3/HER2 tumors and bladder on day 1. Tumor/background (non-targeted tumors, liver, and neck) ratios for Pan-Alexa680(SQ) were significantly higher than the ratios for Pan-Alexa680(ON) for all 4 days (P < 0.01). The tumor/non-targeted tumor, tumor/liver, and tumor/neck ratios on day 4 after injection were 8.1, 10.3, and 8.8 for Pan-Alexa680(SQ), respectively, and 2.7, 3.9, and 4.5 for Pan-Alexa680(ON), respectively. Tra-ICG specifically accumulated in the 3T3/HER2 tumors with very weak fluorescent signal in the liver and intestine. The tumor/background ratios were not significantly different between the mice given Tra-ICG + Pan-Alexa680(SQ) and the mice given Tra-ICG + Pan-Alexa680(ON).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22534030)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22534030)]

No references are currently available.

## References

1 Sano K., Mitsunaga M., Nakajima T., Choyke P.L., Kobayashi H. (2012). In vivo breast cancer characterization imaging using two monoclonal antibodies activatably labeled with near infrared fluorophores. Breast Cancer Res.
2 Kobayashi H., Choyke P.L. (2011). Target-cancer-cell-specific activatable fluorescence imaging probes: rational design and in vivo applications. Acc Chem Res.
3 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
4 Kobayashi H., Ogawa M., Alford R., Choyke P.L., Urano Y. (2010). New strategies for fluorescent probe design in medical diagnostic imaging. Chem Rev.
5 Hama Y., Urano Y., Koyama Y., Kamiya M., Bernardo M., Paik R.S., Shin I.S., Paik C.H., Choyke P.L., Kobayashi H. (2007). A target cell-specific activatable fluorescence probe for in vivo molecular imaging of cancer based on a self-quenched avidin-rhodamine conjugate. Cancer Res.
6 Marras S.A. (2006). Selection of fluorophore and quencher pairs for fluorescent nucleic acid hybridization probes. Methods Mol Biol.
7 Johansson M.K. (2006). Choosing reporter-quencher pairs for efficient quenching through formation of intramolecular dimers. Methods Mol Biol.
8 Okamura Y., Watanabe Y. (2006). Detecting RNA/DNA hybridization using double-labeled donor probes with enhanced fluorescence resonance energy transfer signals. Methods Mol Biol.